# [^111^In]-Labeled divalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX

Chemical name: | [^111^In]-Labeled divalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX
Abbreviated name: | [^111^In]-DOTA-F(ab’)_2_-cG250
Synonym: | [^111^In]-DO3A-F(ab’)_2_-cG250; [^111^In]-F(ab’)_2_-cG250
Agent Category: | Antibody
Target: | Carbonic anhydrase IX
Target Category: | Enzyme
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[[underlined: PubMed]]

A common feature of most solid cancerous tumor types is the presence of hypoxic conditions (1) and the overexpression of carbonic anhydrase IX (CA IX), a transmembrane cell-surface enzyme that is known to regulate the pH and adhesion of tumor cells (2). Hypoxic tumors are often resistant to radio- and chemotherapy, have a high metastatic potential, and usually predict a poor outcome for the cancer patient (3). Although several methods (invasive and noninvasive) are available for the detection of hypoxia in tumors, including the use of radiolabeled small molecules, these methods are not completely reliable because they either yield variable diagnoses or have functional limitations due to incomplete penetration of tumors and fail to detect hypoxia in all tumor types (3, 4). Because CA IX is overexpressed in most solid tumors, it is considered to be a hypoxia biomarker, and targeting the CA IX for the detection of hypoxic tumors is of great interest to investigators (1, 3-5). A ^131^I-labeled murine monoclonal antibody (mAb) that targets the CA IX, designated G250, was developed and evaluated for the radiotherapy of metastatic renal cell carcinoma (RCC) patients, but no major responses were observed because the individuals developed immunity to the mAb (6). Subsequently, a ^131^I-labeled chimeric form of G250, [^131^I]-cG250, was developed and evaluated as an immunotherapeutic agent for the treatment of RCC (7). cG250 has been labeled with other nuclides (such as ^89^Zr, ^177^Lu, ^90^Y, etc.) and has been used in preclinical studies in rats (8) and for the treatment of RCC (7). However, only minor responses were observed in the clinical investigations, and dose escalation studies are ongoing (7).

Radiolabeled antibodies (Abs) have a limited ability to detect or treat cancer because these agents show only a peripheral penetration of solid tumors (due to a large size, ~150 kDa) and leave many neoplastic cells in the lesion untreated (9). In addition, Abs have prolonged blood circulation and present a high radiation dose risk to the bone marrow (10). In comparison, the smaller monovalent Fab (~50 kDa) and the divalent F(ab’)_2_ (~100 kDa) fragments derived from the parent Ab exhibit better tumor penetration and a shorter circulating half-life and are likely to yield better results if used to detect or treat solid malignant tumors (9). Between the two fragment types, the divalent F(ab’)_2_ fragments may be more useful for the detection or treatment of malignant tumors because they have a higher affinity for the antigen (11). With these observations in mind, a divalent F(ab’)_2_ fragment of cG250 was developed, labeled with ^131^I, and compared with the intact [^131^I]-cG250 Ab for its pharmacokinetic behavior and its ability to target tumors in mice and RCC patients (10). However, from this study the investigators concluded that the intact Ab was superior to the divalent fragment for targeting the RCC tumors. A clinical trial to investigate the safety of a ^124^I-labeled version of cG250 in patients with renal masses has been reported (12). In addition, cG250 is also under evaluation in several other clinical trials (http://clinicaltrials.gov/ct2/results?term=cG250). Recently, ^89^Zr-labeled F(ab’)_2_ fragments of cG250 were shown to be suitable for the visualization of hypoxic head and neck cancer xenograft tumors in mice (5).

Brouwers et al. compared the use of [^111^In]-isothiocynate-diethylenetriamine pentaacetic acid-cG250 and [^131^I]-cG250 for the detection of RCC metastases in five patients and concluded that the former tracer was superior to the latter for visualization of the tumors (13). In another study involving three patients, it was shown that neither ^131^I- labeled cG250 nor ^111^In-labeled cG250 were suitable for the radioimmunotherapy of biliary cancer (14). In a recent study using 1,4,7,10-tetraazacyclododecane-N,N’,N'',N’’’-tetraacetic acid (DOTA) as a nuclide conjugating agent, ^111^In-labeled cG250 Ab ([^111^In]-DOTA-cG250) and its Fab ([^111^In]-DOTA-Fab-cG250) and F(ab’)_2_ ([^111^In]-DOTA-F(ab’)_2_-cG250) fragments were generated and compared for their biodistribution and detection of hypoxic HT-29 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (of human colorectal adenocarcinoma origin) xenograft tumors in mice (1).

This chapter details the studies performed with [^111^In]-DOTA-F(ab')_2_-cG250. Studies performed with [^111^In]-DOTA-cG250 (15) and [^111^In]-DOTA-Fab-cG250 (16) are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Carbonic+anhydrase+IX+inhibitors) on carbonic anhydrase IX inhibitors

Human carbonic anhydrase IX in Entrez Gene (http://www.ncbi.nlm.nih.gov/gene/768) (Gene ID 768)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/169636419) of human carbonic anhydrase IX

Crystal structure of the human carbonic anhydrase IX catalytic domain (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=76607)

Human carbonic anhydrase IX in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_omim&IdsFromResult=169636419) database

Hypoxia response in National Cancer Institute-Nature Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100145&pathway_name=hypoxia-inducible%20factor%20in%20the%20cardivascular%20system&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20synthesis&cmd=DetailsSearch)]

The production and labeling of the cG250 F(ab’)_2_ fragment with ^111^In was described in detail by Carlin et al. (1). On average, 4.1 ± 0.2 molecules of DOTA were reported to be conjugated to each molecule of F(ab’)_2_-cG250 (equal to 1.2% DOTA w/w). The ^111^In-labeling efficiency of the cG250 Fab fragment was >90% with a radiochemical purity of >99.9% and a specific activity of 370 MBq/mg (~1.5 Ci/mg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20in%20vitro&cmd=DetailsSearch)]

Using SKRC-38 cells (of human RCC origin) under in vitro conditions, the immunoreactivity of [^111^In]-DOTA-F(ab’)_2_-cG250 was >90% with a B_max_ of 114,000 ± 19,000 binding sites/cell (1). Under the same experimental conditions, the B_max_ values for the cG250 and its Fab fragment were 120,000 ± 22,000 and 118,000 ± 21,000 binding sites/cell, respectively (1). [^111^In]-DOTA-F(ab’)_2_-cG250 was reported to have a K_d_ of 1.76 ± 0.08 nM for the CA IX on the SKRC-38 cells. In comparison, the K_d_ values for the ^111^In-labeled cG250 and the Fab fragment were 2.48 ± 0.04 and 14.05 ± 0.47 nM, respectively.

The tumor uptake of radioactivity from the labeled F(ab’)_2_, cG250, and the Fab fragment was confirmed with ex vivo autoradiography of the tumor sections (1). In addition, the expression of CA IX and the occurrence of hypoxic conditions in the tumor sections were confirmed with immunohistochemical and pimonidazole staining procedures, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DOTA-F(ab’)_2_-cG250 was studied in nu/nu nude mice (n = 4–5 animals/group per time point) bearing hypoxic HT-29 colorectal tumor xenografts as described by Carlin et al. (1). The animals were injected with the ^111^In-labeled F(ab’)_2_ fragment through the tail vein and euthanized at preselected time points (ranging from 6 h to 7 days post-injection (p.i.)) to determine the amount of radioactivity accumulated in the tumors and the major organs. Data generated from the study were presented as percent injected dose per gram tissue (% ID/g).

The accumulation of radioactivity in the tumors with the ^111^In-labeled F(ab’)_2_ fragment was 7.6 ± 1.4% ID/g and 9.3 ± 2.1% ID/g at 6 h and 24 h p.i., respectively. The tumor/muscle (TM) and tumor/blood (TB) ratios with the divalent tracer were 8.9 and 4.6, respectively at 24 h p.i. Compared with the labeled F(ab’)_2_ fragment, the tumor uptake of radioactivity from the labeled Fab fragment was 3.6 ± 1.3% ID/g and 3.5 ± 1.7% ID/g at 6 and 24 h p.i., respectively. The TM and TB ratios with the ^111^In labeled monovalent fragment were 4.8 and 2.8, respectively, at 6 h p.i., and these ratios increased to 6.7 and 16.6, respectively, at 24 h p.i. The TM and TB ratios obtained with the two Ab fragments were lower than those observed with [^111^In]-DOTA-cG250 at 7 days p.i. (see below). The tumor uptake of ^111^In-labeled cG250 was 20.1 ± 4.8% ID/g at 2 days p.i. and increased to 26.4 ± 5.7% ID/g at day 7. In general, the tumor/non-tumor (TNT) ratios with [^111^In]-DOTA-cG250 increased for all tissues up to 7 days p.i., except for the liver and spleen, and little change in the TNT ratio for these organs was apparent during this period. At 7 days p.i., the TM and TB ratios with the labeled cG250 were 69 and 6.6, respectively, indicating a slow washout of radioactivity from these organs. The two Ab fragments showed ~10-fold lower tumor uptake and a similar increase in kidney accumulation of radioactivity compared with [^111^In]-DOTA-cG250. A high accumulation of radioactivity in the kidney was expected with the Fab and F(ab’)_2_ fragments because these Ab derivatives (or their breakdown products) are known to be excreted through the urinary route and these organs express a high level of CA IX. These observations suggested that clearance of the [^111^In]-DOTA-Fab-cG250 and the [^111^In]-DOTA-F(ab’)_2_-cG250 fragments from blood was faster than that of the intact [^111^In]-DOTA-cG250 Ab. These results indicated that cG250 had a long circulation time compared with the Fab and F(ab’)_2_ fragments and that the tumor had a superior retention of the labeled Ab compared to either of its fragments. No blocking studies were reported.

From these studies, the investigators concluded that imaging with [^111^In]-DOTA-cG250 at 7 days p.i. was a better and more sensitive method for the detection of CA IX in hypoxic tumors in a murine model compared with its ^111^In-labeled Fab or F(ab’)_2_ fragments (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

National Institutes of Health grants P01 CA115675, P01 CA033049 and P50 CA086438

## References

1 Carlin S., Khan N., Ku T., Longo V.A., Larson S.M., Smith-Jones P.M. (2010). Molecular targeting of carbonic anhydrase IX in mice with hypoxic HT29 colorectal tumor xenografts. PLoS One.
2 De Simone G., Supuran C.T. (2010). Carbonic anhydrase IX: Biochemical and crystallographic characterization of a novel antitumor target. Biochim Biophys Acta.
3 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging. 2010
4 Mees G., Dierckx R., Vangestel C., Van de Wiele C. (2009). Molecular imaging of hypoxia with radiolabelled agents. Eur J Nucl Med Mol Imaging.
5 Hoeben B.A., Kaanders J.H., Franssen G.M., Troost E.G., Rijken P.F., Oosterwijk E., van Dongen G.A., Oyen W.J., Boerman O.C., Bussink J. (2010). PET of hypoxia with 89Zr-labeled cG250-F(ab')2 in head and neck tumors. J Nucl Med.
6 Divgi C.R., Bander N.H., Scott A.M., O'Donoghue J.A., Sgouros G., Welt S., Finn R.D., Morrissey F., Capitelli P., Williams J.M., Deland D., Nakhre A., Oosterwijk E., Gulec S., Graham M.C., Larson S.M., Old L.J. (1998). Phase I/II radioimmunotherapy trial with iodine-131-labeled monoclonal antibody G250 in metastatic renal cell carcinoma. Clin Cancer Res.
7 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
8 Brouwers A., Verel I., Van Eerd J., Visser G., Steffens M., Oosterwijk E., Corstens F., Oyen W., Van Dongen G., Boerman O. (2004). PET radioimmunoscintigraphy of renal cell cancer using 89Zr-labeled cG250 monoclonal antibody in nude rats. Cancer Biother Radiopharm.
9 Schmidt M.M., Wittrup K.D. (2009). A modeling analysis of the effects of molecular size and binding affinity on tumor targeting. Mol Cancer Ther.
10 Brouwers A., Mulders P., Oosterwijk E., Buijs W., Corstens F., Boerman O., Oyen W. (2004). Pharmacokinetics and tumor targeting of 131I-labeled F(ab')2 fragments of the chimeric monoclonal antibody G250: preclinical and clinical pilot studies. Cancer Biother Radiopharm.
11 Rudnick S.I., Adams G.P. (2009). Affinity and avidity in antibody-based tumor targeting. Cancer Biother Radiopharm.
12 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.
13 Brouwers A.H., Buijs W.C., Oosterwijk E., Boerman O.C., Mala C., De Mulder P.H., Corstens F.H., Mulders P.F., Oyen W.J. (2003). Targeting of metastatic renal cell carcinoma with the chimeric monoclonal antibody G250 labeled with (131)I or (111)In: an intrapatient comparison. Clin Cancer Res.
14 Hendrickx B.W., Punt C.J., Boerman O.C., Postema E.J., Oosterwijk E., Mavridu A., Corstens F.H., Oyen W.J. (2006). Targeting of biliary cancer with radiolabeled chimeric monoclonal antibody CG250. Cancer Biother Radiopharm.
15 Chopra, A., [111In]-Labeled chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
16 Chopra, A., [111In]-Labeled monovalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.